# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser-NH_2_ (AE105-NH_2_)

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser-NH_2_ (AE105-NH_2_)
Abbreviated name: | ^64^Cu-DOTA-AE105-NH_2_, ^64^Cu-DOTA-D-Cha-F-s-r-Y-L-W-S-NH_2_
Synonym:
Agent category: | Peptide
Target: | Urokinase-type plasminogen activator receptor (uPAR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=48146021), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48146020) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=5329) for more information about uPAR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM (3). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7).

Urokinase-type plasminogen activator (uPA) is a serine protease (8, 9). The uPA/uPA receptor (uPAR) system is responsible for tissue degradation after plasminogen activation to plasmin, which leads to a cascade of proteolysis or thrombolysis, depending on the physiological conditions. uPA also directly activates MMPs, vascular endothelial growth factor, and human growth factor (10). Malignant tumors often express high levels of uPA and uPAR (11); therefore, the uPA/uPAR system is linked to vascular diseases and cancer. The synthetic peptide Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser (AE105) has been identified to have a high affinity (dissociation constant for human uPAR (K_d_) = 0.4 nM) (12), and AE105 has been labeled with ^64^Cu (T_1/2_ = 12.7 h, β^+^ = 17.8%) as ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-AE105 (^64^Cu-DOTA-AE105) for use in positron emission tomography (PET) imaging of uPAR expression in tumors (13). Persson et al. (14) extended the evaluation of AE105 in PET and biodistribution studies with ^64^Cu-DOTA-AE105-NH_2_.

### Related Resource Links

- Chapters in MICAD (uPAR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=uPAR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (uPAR (http://www.ncbi.nlm.nih.gov/gene/5329), uPA (http://www.ncbi.nlm.nih.gov/gene/5328))
- Articles in Online Mendelian Inheritance in Man (OMIM) (uPAR (http://omim.org/entry/173391), uPA (http://omim.org/entry/191840))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+synthesis)]

Persson et al. (14) performed DOTA chelation of the N-terminus of AE105-NH_2_via solid-phase synthesis. A mixture of AE105-NH_2_ and DOTA-tris(tBu)ester in a molar ratio of 1:3 was incubated for 24–48 h at room temperature. The DOTA-AE105-NH_2_ conjugate was purified with high-performance liquid chromatography (HPLC). The number of DOTA molecules per peptide was ~1 as determined with mass spectroscopy. For radiolabeling, DOTA-AE105-NH_2_ (2 nmol) was added to 150 MBq (4 mCi) ^64^CuCl_2_ diluted in 0.1 M ammonium acetate buffer (pH 8.0). The reaction mixture was incubated for 1 h at 70ºC with a radiolabeling yield of >90%. ^64^Cu-DOTA-AE105-NH_2_ was purified with a Sep-Pak cartridge (>95% radiochemical purity). ^64^Cu-DOTA-AE105_mut_-NH_2_, used as an inactive control, was prepared similarly. The specific activities of ^64^Cu-DOTA-AE105 and ^64^Cu-DOTA-AE105_mut_-NH_2_ were ~25 GBq/μmol (0.68 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+and+in+vitro)]

Persson et al. (14) performed binding experiments with AE105-NH_2_, DOTA-AE105-NH_2_, and inactive DOTA-AE105_mut_-NH_2_ with the use of a Biacore sensor chip immobilized with pro-uPA. The IC_50_ values for inhibiting the binding of uPAR (0.5 nM) to pro-uPA were 7.6 ± 2.0 nM, 6.7 ± 0.9 nM, and >10 µM for AE105-NH_2_, DOTA-AE105-NH_2_, and inactive DOTA-AE105_mut_-NH_2_, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+rodentia)]

Persson et al. (14) performed ex vivo biodistribution studies at 4.5 h after injection of ^64^Cu-DOTA-AE105-NH_2_ or ^64^Cu-DOTA-AE105_mut_-NH_2_ in mice (n = 3/group) bearing U87MG human glioblastomas (uPAR-positive). The accumulation levels of ^64^Cu-DOTA-AE105-NH_2_ and ^64^Cu-DOTA-AE105_mut_-NH_2_ in the U87MG tumors were 4.2 ± 0.8% injected dose per gram (ID/g) and 1.2 ± 0.1% ID/g, respectively. The accumulation of both tracers was similar in the normal organs, with the highest accumulation of radioactivity in the liver (11%–14% ID/g) and kidneys (~6% ID/g). The tumor/blood and tumor/muscle ratios for ^64^Cu-DOTA-AE105-NH_2_ were 3.5 and 14.0, respectively. The tumor/blood and tumor/muscle ratios for ^64^Cu-DOTA-AE105_mut_-NH_2_ were 1.2 and 4.3, respectively.

PET imaging studies were performed at 1, 4.5, and 22 h after injection of ^64^Cu-DOTA-AE105-NH_2_ or ^64^Cu-DOTA-AE105_mut_-NH_2_ in mice bearing U87MG tumors (n = 3/group) (14). The tumors were clearly visualized for ^64^Cu-DOTA-AE105-NH_2_ at all three time points, with 5%–6% ID/g. ^64^Cu-DOTA-AE105-NH_2_ exhibited a significantly higher (P < 0.001) tumor accumulation than ^64^Cu-DOTA-AE105_mut_-NH_2_ (1.6%–2.2% ID/g). Pretreatment (5 min) with 2 nmol DOTA-AE105-NH_2_ before ^64^Cu-DOTA-AE105-NH_2_ injection inhibited the tumor accumulation by 78% at 4.5 h after injection (P < 0.001).

Persson et al. (14) performed ^64^Cu-DOTA-AE105-NH_2_ PET imaging in mice (n = 4/group) bearing H727 (low uPAR expression), HT-29 (moderate uPAR expression), or U87Mg (high uPAR expression) xenografts at 1, 4.5, and 22 h after injection. There was a significant correlation (R^2^ = 0.73; P < 0.001) between tumor accumulation and uPAR expression at these time points. In another experiment, the tumor accumulation of [^18^F]FDG and ^64^Cu-DOTA-AE105-NH_2_ was compared in mice bearing H727 and U87MG tumors at 1 h after injection. The tumor accumulation of FDG was similar in H727 (1.52 ± 0.03% ID/g) and U87MG (1.97 ± 0.18% ID/g) tumors, whereas the tumor accumulation of ^64^Cu-DOTA-AE105-NH_2_ was significantly (P < 0.05) higher in U87MG (3.88 ± 0.74% ID/g) than in H727 tumors (1.71 ± 0.11% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Choong P.F., Nadesapillai A.P. (2003). Urokinase plasminogen activator system: a multifunctional role in tumor progression and metastasis. Clin Orthop Relat Res.
9 Rabbani S.A., Mazar A.P. (2001). The role of the plasminogen activation system in angiogenesis and metastasis. Surg Oncol Clin N Am.
10 Folkman J., Shing Y. (1992). Angiogenesis. J Biol Chem.
11 Duffy M.J., Maguire T.M., McDermott E.W., O'Higgins N. (1999). Urokinase plasminogen activator: a prognostic marker in multiple types of cancer. J Surg Oncol.
12 Ploug M., Ostergaard S., Gardsvoll H., Kovalski K., Holst-Hansen C., Holm A., Ossowski L., Dano K. (2001). Peptide-derived antagonists of the urokinase receptor. affinity maturation by combinatorial chemistry, identification of functional epitopes, and inhibitory effect on cancer cell intravasation. Biochemistry.
13 Li Z.B., Niu G., Wang H., He L., Yang L., Ploug M., Chen X. (2008). Imaging of urokinase-type plasminogen activator receptor expression using a 64Cu-labeled linear peptide antagonist by microPET. Clin Cancer Res.
14 Persson M., Madsen J., Ostergaard S., Jensen M.M., Jorgensen J.T., Juhl K., Lehmann C., Ploug M., Kjaer A. (2012). Quantitative PET of human urokinase-type plasminogen activator receptor with 64Cu-DOTA-AE105: implications for visualizing cancer invasion. J Nucl Med.